# m-Cyano-p-[^18^F]fluorohippurate

Chemical name: | m-Cyano-p-[^18^F]fluorohippurate
Abbreviated name: | [^18^F]-CNPFH
Synonym:
Agent Category: | Compound
Target: | Organic anion transporter 1 (OAT1)
Target Category: | Transporter
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on above structure of [^18^F]CNPFH for more information in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=fluorohippurate&cmd=DetailsSearch)]

Although ortho-[^131^I]-iodohippurate ([^131^I]-OIH) is considered a gold standard for renal plasma flow imaging and provides quantitative results with single-photon emission tomography (SPECT), images produced with this agent are not superior to those obtained with either ^99m^Tc-labeled mercaptoacetylglycylglycylglycine ([^99m^Tc]-MAG_3_) which is secreted by the renal proximal tubules or ^99m^Tc-labeled diethylenetriamine pentaacetic acid ([^99m^Tc]-DTPA), which is filtered by the glomeruli (1). As a consequence, based on the superior imaging properties of ^99m^Tc, [^99m^Tc]-MAG_3_ is often used with planar gamma imaging in the clinic to evaluate kidney function and perform renal scans (renography) (2). However, even with these radiolabeled compounds, a low signal/background ratio is obtained from the kidneys due to a differential attenuation of the ^99m^Tc-gamma radiation between the two organs. In addition, the quantitative data generated with this tracer are of poor quality. Therefore, investigators are evaluating the use of dynamic SPECT or positron emission tomography (PET) to assess kidney function and/or renography because these modalities provide substantially superior quantitative results compared to planar imaging. PET offers several benefits over SPECT for renography because PET has higher spatial resolution and sensitivity, shows minimal differential signal attenuation between the kidneys, and can be used for real-time acquisition of the dynamic images (3). In an effort to develop an alternate tracer that can be used to evaluate kidney function and perform renography with PET, para-^18^F-fluorohippurate ([^18^F]-PFH), a renal tubular agent, was identified as a potential candidate by Awasthi et al. (3). The investigators hypothesized that [^18^F]-PFH could be a superior PET renal imaging agent compared to [^99m^Tc]-MAG_3_ because of its pharmacokinetic and imaging characteristics. In a preliminary investigation, it was shown that [^18^F]-PFH was suitable for renography in normal rats and that high-quality dynamic PET images could be obtained from the animals (3).

The synthesis of [^18^F]-PFH was done with a two-pot four-step procedure, but in view of the short half-life of ^18^F (~110 min), and to make sure that the tracer is available quickly for use in the clinic, it is necessary to reduce the total time required to produce the labeled compound (4). Therefore, a new hippurate analog, m-cyano-p-[^18^F]fluorohippurate ([^18^F]-CNPFH), was synthesized with a single-step procedure. The biodistribution and renography properties of this labeled compound were studied in rats and compared with those of [^18^F]PFH (4).

### Related Resource Links

Related chapter in MICAD (http://www.ncbi.nlm.nih.gov/books/NBK52894/)

References for [^131^I]-iodohippurate in PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=131I-iodohippurate&cmd=DetailsSearch)

References for [^99m^Tc]-MAG_3_ in PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc-MAG3&cmd=DetailsSearch)

Clinical trials (http://clinicaltrials.gov/ct2/results?term=99mTc-MAG3+) with [^99m^Tc]-MAG_3_

References for [^99m^Tc]-DTPA in PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc-DTPA&cmd=DetailsSearch)

Clinical trials (http://clinicaltrials.gov/ct2/results?term=99mTc-DTPA) with [^99m^Tc]-DTPA

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B18%20F%5DCNPFH%20synthesis&cmd=DetailsSearch)]

The one-step nucleophilic aromatic substitution synthesis of CNPFH and its labeling with ^18^F has been described by Pathuri et al. (4). The radiochemical yield (RCY) of the purified tracer was 73.2 ± 0.6% based on the amount of ^18^F added to three independent synthesis reactions. The radiochemical purity (RCP) of the labeled compound was >99% as determined with reverse-phase high-performance liquid chromatography (RP-HPLC). The total time of synthesis (TOS) and specific activity (SA) of [^18^F]-CNPFH were not reported. After purification, the tracer was dried, reconstituted in 0.9% sodium chloride, and sterilized by passing through a 0.22-μm syringe filter.

For comparison purposes, [^18^F]-PFH was also used in some studies; however, the RCY, RCP, and SA of this tracer were not reported (4). In an earlier study, the RCY and RCP of [^18^F]-PFH were reported to be 91%–95% and >99%, respectively, as determined with radio-HPLC (3). The TOS and the SA of ^18^F-PFH were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B18%20F%5DCNPFH%20in%20vitro%20studies&cmd=DetailsSearch)]

No degradation products of [^18^F]-CNPFH were generated (as determined with HPLC) when the tracer was incubated in vitro with human plasma for at least 1 h at 37ºC (4).

HPLC analysis of urine obtained from a rat at 30 min after injection of [^18^F]-CNPFH showed that no metabolites of the radiochemical were present in the sample (4).

These studies indicated that [^18^F]-CNPFH was stable under in vitro and in vivo conditions.

The in vivo plasma protein binding and erythrocyte uptake of [^18^F]-CNPFH were reported to be 46.1% and 16.3%, respectively (4). These values were similar to those reported earlier for [^18^F]-PFH (3).

The partition coefficients of [^18^F]-CNPFH and [^18^F]-PFH in a water/n-octanol mixture (at pH 7.0) were determined to be −2.54 ± 0.23 and −2.53 ± 0.08, respectively (4).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B18%20F%5DCNPFH%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^18^F]-CNPFH was studied in normal Sprague-Dawley rats as described elsewhere (4). Briefly, the animals (n = 4 rats/time point; under anesthesia) were injected with ~0.4 MBq (~15 μCi) [^18^F]-CNPFH through the tail vein, and the rodents were euthanized at 10 min postinjection (p.i.) or 1 h p.i. to retrieve all the organs of interest. Subsequently, the amount of radioactivity accumulated in the various tissues was determined (Table 1). Data obtained from the study were presented as percent of injected dose per gram tissue (% ID/g).

Table 1: Biodistribution of [ ^ 18 ^ F]-CNPFH in rats at 10 min p.i. and 1 h p.i.

Organ | Uptake of radioactivity (% ID/g)
Organ | 10 min p.i. | 1 h p.i.
Blood | 0. 70 ± 0.13 | 0.03 ± 0.02
Heart | 0.17 ± 0.02 | 0.00 ± 0.01
Lung | 0.25 ± 0.05 | 0.01 ± 0.01
Liver | 0.67 ± 0.03 | 0.04 ± 0.02
Spleen | 0.11 ± 0.04 | 0.01 ± 0.02
Kidney | 12.50 ± 1.10 | 0.44 ± 0.23
Muscle | 0.06 ± 0.01 | 0.00 ± 0.00
Intestine | 0.49 ± 0.47 | 0.89 ± 0.35
Urine* | 37.20 ± 8.90 | 62.00 ± 11.30

*Data presented as % ID. ID, injected dose; p.i., postinjection. For complete data set see Pathuri et al. ( 4 ).

The tracer was rapidly cleared from blood circulation (0.70 ± 0.13% ID/g at 10 min p.i. and 0.03 ± 0.02% ID/g at 1 h p.i.), and a similar trend was noticed with all the major organs (4). The amount of radioactivity in the intestine increased from 0.49 ± 0.47% ID/g at 10 min p.i. to 0.89 ± 0.35% ID/g at 1 h p.i. The amount of label in the kidneys decreased from 12.50 ± 1.10% ID/g at 10 min p.i. to 0.44 ± 0.23% ID/g at 1 h p.i., and the level of tracer in the urine was 37.20 ± 8.90% ID and 62.00 ± 11.30% ID at 10 min p.i. and 1 h p.i., respectively. This indicated that, although a major portion of radioactivity was excreted through the renal route, some portion of the tracer was cleared through the hepatobiliary system.

Dynamic PET/computed tomography (CT) imaging with [^18^F]-CNPFH and [^18^F]-PFH was performed on 4 rats on two separate days (4). On the first day, the animals were injected with ~2.7 MBq (~100 μCi) [^18^F]-CNPFH for imaging. For comparison, the same animals were injected with an equal amount of [^18^F]-PFH for imaging on the second day. Whole-body PET scans of the animals were acquired for 30 min p.i., followed by CT imaging for 1 min. Using appropriate software, regions of interest were drawn on the images to delineate the kidneys, and a renogram analysis was performed for each rat. From the renograms it was determined that the peak activity times for [^18^F]-CNPFH and [^18^F]-PFH in the animals were 3.2 ± 0.4 min and 2.9 ± 0.4 min, respectively. The time to half-maximal activity was determined to be significantly higher (P = 0.03) for [^18^F]-CNPFH (11.4 ± 2.8 min) than for [^18^F]-PFH (7.1 ± 1.3 min). The PET images obtained with [^18^F]-CNPFH showed some accumulation of radioactivity in the liver and intestine, but no label was detected in these organs of animals injected with [^18^F]-PFH.

From these studies, the investigators concluded that, although [^18^F]-CNPFH was comparable to [^18^F]-PFH to determine the renal function in rats, it produced some background signal in the PET images of the animals (4).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B18%20F%5DCNPFH%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No reference is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B18%20F%5DCNPFH%20Non-Human%20Primates&cmd=DetailsSearch)]

No reference is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B18%20F%5DCNPFH%20Human%20Studies&cmd=DetailsSearch)]

No reference is currently available.

## Supplemental Information

[Disclaimers]

No reference is currently available.

## References

1 Itoh K. (2001). 99mTc-MAG3: review of pharmacokinetics, clinical application to renal diseases and quantification of renal function. Ann Nucl Med.
2 Taylor A., Eshima D., Fritzberg A.R., Christian P.E., Kasina S. (1986). Comparison of iodine-131 OIH and technetium-99m MAG3 renal imaging in volunteers. J Nucl Med.
3 Awasthi V., Pathuri G., Agashe H.B., Gali H. (2011). Synthesis and in vivo evaluation of p-18F-Fluorohippurate as a new radiopharmaceutical for assessment of renal function by PET. J Nucl Med.
4 Pathuri G., Hedrick A.F., Awasthi V., Gali H. (2012). Single-step radiosynthesis and in vivo evaluation of a novel fluorine-18 labeled hippurate for use as a PET renal agent. Nucl Med Biol.